# [N-^11^C-methyl]-[4-[(4-Methyl-1-piperazinyl)methyl]-N-[4-methyl-3-[[4-(3-pyridyl)-2-pyrimidinyl]amino]phenyl]benzamide

Chemical name: | [N-^11^C-methyl]-[4-[(4-Methyl-1-piperazinyl)methyl]-N-[4-methyl-3-[[4-(3-pyridyl)-2-pyrimidinyl]amino]phenyl]benzamide
Abbreviated name: | [N-^11^C-methyl]imatinib
Synonym:
Backbone: | Compound
Target: | Various tyrosine kinases
Mechanism: | Competitive inhibitor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | Not required
Studies: | - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gleevec&WebEnv=0Wx7pD8O_LVwdWwQluKD-ZWvXgAt95xZ0dsWXnsYKHWNZ_h5hLcicXnuOHCAtYE6mws5iVJTj566sZ%40D476257165EDE870_0070SID&WebEnvRq=1)]

Imatinib ([4-[(4-methyl-1-piperazinyl)methyl]-N-[4-methyl-3-[[4-(3-pyridyl)-2-pyrimidinyl]amino]phenyl]benzamide) is a synthetic tyrosine kinase (TK) signal transduction inhibitor used for the treatment of a variety of chronic myeloid leukemia (CML) attributed to the Philadelphia chromosome–positive trait (1). This chromosomal abnormality develops after a genetic translocation between chromosome 9 and chromosome 22, which leads to the expression of an abnormal bcr-abl TK that is no longer dependent on normal activation as a result of the interaction between interleukin-3 and its receptor. This drug is also used for the treatment of gastrointestinal stromal tumors (GIST) that are caused by mutations in the closely related c-kit or platelet-derived growth factor (PDGF) TKs (2). In addition, imatinib has been shown to be an effective treatment against a variety of other conditions that are characterized by the expression of abl, c-kit, or PDGF TKs (3). Although imatinib is a useful chemotherapeutic agent for the treatment of CML and GIST, patients undergoing therapy for these conditions often develop resistance to the drug as a result of secondary mutations in the TKs.

The FDA approved imatinib for the treatment of CML in May 2001 and subsequently for the treatment of GIST in January 2002 (4). A detailed description of the indications for which imatinib can be prescribed is available in the product insert from the manufacturer (5).

In an attempt to initiate understanding of the development of drug resistance to imatinib, an N-[^11^C]-methyl derivative of imatinib was synthesized. The radiolabeled compound was then administered to baboons (Papio anubis) to determine drug biodistribution and pharmacokinetics in the animals (3).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=carbon-11-labeled+imatinib+synthesis&WebEnv=0DCxxUUPRxTOGMGl54qnEtKAWSIUHGp1PeAJ9wRIx8kZengSbx643na_cRRJeJ-fHLIk7NlwUABq-I%40D476257165EDE870_0070SID&WebEnvRq=1)]

The synthesis of imatinib has been described by Kil et al. (3). Briefly, [4-[(4-benzyloxycarbonyl-1-piperazinyl)methyl]-N-[4-methyl-3-[[4-(3-pyridyl)-2-pyrimidinyl]amino]phenyl]benzamide was prepared by via amide bond formation between N-(5-amino-2-methylphenyl)-4-(3-pyridyl)-2-pyrimidinamine and benzyl 4-(4’-hydroxycarbonylbenzyl)-1-piperazinecarboxylate. The yield of this reaction was 54%. The compound was then used to prepare norimatinib by use of a procedure modified from that of Baker et al. (6).

To radiolabel the agent, norimatinib in dimethyl sulfoxide was mixed with ^11^C-labeled methyl iodide. When the radioactivity as determined with a sodium iodide detector peaked in the reaction vessel, the vessel was sealed and heated at 80°C for 10 min in an oil bath. The reaction mixture was then diluted in 0.06 N hydrochloric acid (HCl) and the product was isolated by high-performance liquid chromatography (HPLC) on a Luna semi-preparative C18 column. The product was transferred to a rotary evaporator containing 1 N HCl and the solvent was allowed to co-evaporate. The resulting residue was dissolved in saline and filtered through a 0.22-µm filter in a sterile vial for positron emission tomography (PET) studies.

The radiochemical purity of the labeled product as determined by thin-layer chromatography and HPLC was >98%. The synthesis time was 1 h from the end of bombardment. Specific activity of the radiochemical ranged from 40.7–51.8 GBq/µmol (1.1–1.4 Ci/µmol) at the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B11C-methyl%5Dimatinib+imaging+in+vitro&WebEnv=0gk-nKYNp5da46d6WyAnGKHhVE4B6s6JCdezcFJKBlDzvdi7cogRngg3AqSqbbUiOVS1PdXNf5Oh9s%40D4754F2F6601DD70_0122SID&WebEnvRq=1)]

No publications are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B11C-methyl%5Dimatinib+imaging+rodentia&WebEnv=0Mqa3tGJ_q0FyVXaNERrujHznSJaU1aWkEJkTNJ4GVxbNVS71wmQ28mwUZr42CEmQupv-7yKTQAL7A%40D4754F2F6601DD70_0122SID&WebEnvRq=1)]

No publications are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%5B11C-methyl%5Dimatinib+imaging+Other+Non-Primate+Mammals&WebEnv=08XvSHidLXl-DLJmtn-b1qWwlfCm-1fDxKnsUokybECPA9c-ARssKhOps6_poM3JDLPEGR_KGsWgva%40D4754F2F6601DD70_0122SID&WebEnvRq=1)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=imatinib+imaging+in+baboons&WebEnv=08SEOul3XxOxGmnDoM-mJcwYOsiLMJGwE6hNXGPfzKgkT0ktdcuXpsaljIhK3BP8FUkF1HWJgEo1jj%40D4754F2F6601DD70_0122SID&WebEnvRq=1)]

PET studies with [N-^11^C-methyl]imatinib were performed in baboons (3). Two i.v. injections of the radiochemical were administered to each animal and the animals were scanned twice. The second scan was performed 2 h after the first scan. From the PET images it was evident that the radiochemical was not taken up by the brain or concentrated in the sinuses and tissue surrounding the brain. A P-glycoprotein–mediated efflux was suggested to contribute to elimination of the [N-^11^C-methyl]imatinib from the blood–brain barrier and also for development of resistance to the drug (7). The radiolabel was concentrated primarily in the liver, kidney, and gallbladder after the injections. The radioactivity from [N-^11^C-methyl]imatinib and/or its metabolites peaked early in the heart, lungs, and spleen and cleared rapidly from these organs. In the liver and kidneys, the label peaked and cleared more slowly, and it accumulated over time in the gallbladder. The accumulation of ^11^C in the gallbladder indicated the excretion of imatinib and its metabolites through the gastrointestinal tract.

A rapid clearance of imatinib and its metabolites was observed in the plasma. Treatment of the animals with [N-^11^C-methyl]imatinib after administration of unlabeled imatinib reduced the uptake in the heart, lungs, kidneys, and spleen at the early time points, but paralleled one another after 40 min. During the same period the uptake was higher in the liver and gallbladder after the pretreatment. When the uptake in the liver, kidneys, and spleen were normalized for plasma, no difference in the uptake was noticed, indicating that the reduction in uptake was driven by the reduction in plasma. The normalized time-activity curves for liver and gallbladder showed an increase in uptake of the label, indicating an increased accumulation of the drug metabolites in these organs.

It was concluded that [N-^11^C-methyl]imatinib can be used to assess the distribution and kinetics of imatinib in humans and to determine whether it can target tumors. It may also be used to help plan a chemotherapy regimen for a patient, to monitor treatment response, and to investigate the development of drug resistance.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=imatinib+imaging+human+studies&WebEnv=096xmLGp5rYNB1xHjMB1vipFEsAlFp9PdTrm0Yh2qS9eB8ZaeDUjblJUXQo99azDQr95iiijgEpc55%40D4754F2F6601DD70_0122SID&WebEnvRq=1)]

No publications are currently available.

## References

1 Moen M.D., McKeage K., Plosker G.L., Siddiqui M.A. (2007). Imatinib: a review of its use in chronic myeloid leukaemia. Drugs.
2 Rubin B.P., Heinrich M.C., Corless C.L. (2007). Gastrointestinal stromal tumour. Lancet.
3 Kil K.E., Ding Y.S., Lin K.S., Alexoff D., Kim S.W., Shea C., Xu Y., Muench L., Fowler J.S. (2007). Synthesis and positron emission tomography studies of carbon-11-labeled imatinib (Gleevec). Nucl Med Biol.
4 Collins, J.M., J.R.W. Klecker, and L.W. Anderson, Imaging of drug accumulation as a guide to antitumor therapy. Patent number 7,175,830., U.S.P. Office, Editor. 2007, The United States of America Secretary of Health and Human Services
5 . Novartis, Gleevec2006, Novartis Pharma Stein AG: Stein, Switzerland.
6 Baker P.L., Gendler P.L., Rapoport H. (1981). Acylation of dibasic compounds containing amino amidine and aminoguanidine functions. J Organic Chem.
7 Mahon F.X., Deininger M.W., Schultheis B., Chabrol J., Reiffers J., Goldman J.M., Melo J.V. (2000). Selection and characterization of BCR-ABL positive cell lines with differential sensitivity to the tyrosine kinase inhibitor STI571: diverse mechanisms of resistance. Blood.